# N-Methyl-[^11^C]-2-(4'-methylaminophenyl)-6-hydroxybenzothiasole

Chemical name: | N-Methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole
Abbreviated name: | [^11^C]6-OH-BTA-1, [^11^C]PIB
Synonym: | [^11^C]Pittsburgh Compound-B
Backbone: | Compound
Target: | Aggregates of Amyloid-beta peptide
Mechanism: | Acceptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions overtime (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-beta peptides consisting of 40 to 42 amino acids) and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single photon emission computed tomography (SPECT), and positron emission tomography (PET) (8-13). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Out of these analogues, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal-to-noise ratios for PET imaging, because it is highly lipophilic. N-Methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for the senile plaques in the brain (16).

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), tau (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=tau+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351), tau (http://www.ncbi.nlm.nih.gov/gene/4137)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/104760), tau (http://www.ncbi.nlm.nih.gov/omim/157140))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid), [^11^C]PIB (http://www.clinicaltrials.gov/ct2/results?term=PIB&Search=Search))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20synthesis)]

[^11^C]6-OH-BTA-1 was readily synthesized by standard ^11^C-methylation of 2-(4’-aminophenyl)-6-methoxymethoxybenzothiazole with [^11^C]methyl iodide, followed by hydrolysis (15). The radiochemical yield averaged 12.1% at the end of synthesis based on [^11^C]methyl iodide, and the specific activity averaged 85 GBq/μmol (2.3 Ci/μmol) at the end of synthesis. Radiochemical and chemical purities were >95% as determined by high-performance liquid chromatography (HPLC).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20in%20vitro)]

6-OH-BTA-1 has a binding affinity (K_i_) of 4.5 nM for aggregated amyloid-beta(1-40) fibrils in competition with [N-methyl-^3^H]BTA-1 (15). The K_i_ Value for thioflavin-T was found to be 580 nM. Saturation binding studies with [N-methyl-^3^H]6-OH-BTA-1 to amyloid-beta(1-40) peptide showed a K_d_ value of 4.7 nM and a B_max_ value of 2.7 pmol of 6-OH-BTA-1 per nmol of amyloid-beta(1-40) peptide. 6-OH-BTA-1 showed no inhibition in an array of neurotransmitter receptor and transporter assays. Saturation binding studies with [N-methyl-^3^H]6-OH-BTA-1 to homogenates of frontal cortex from postmortem advanced AD brain showed a K_D_ value of 1.4 nM and a B_max_ value of 1900 pmol per g tissue. There was no specific binding of [N-methyl-^3^H]6-OH-BTA-1 to homogenates of frontal cortex from age-matched control brain as well as to homogenates of cerebellum from AD brain or control brain. Klunk et al (16) showed that [^11^C]6-OH-BTA-1 bound specifically to frontal cortex of postmortem AD brain slices, and its binding could be blocked by excess unlabeled BTA-1. There was little binding of [^11^C]6-OH-BTA-1 to frontal cortex of normal elderly control brain slices.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20rodentia)]

[^11^C]-labeled BTA derivatives (0.37-3.7 MBq, 10-100 μCi) were injected intravenously into mice to study their accumulation into brain of normal mice (15). 6-OH-BTA-1 has an apparent lipophilicity (log P_c18_) of 1.2. It is expected to enter the brain readily. The radioactivity in excised brain samples was measured at 2 and 30 min after injection. [^11^C]6-OH-BTA-1 showed the lowest 30-min brain value of 0.018% injected dose (ID)-kg/g, with the highest 2 min-to-30 min ratio of 12. [^11^C]BTA-1 was the second best tracer, with a 2 min-to-30 min ratio of 7.6. The peripheral metabolism of [^11^C]6-OH-BTA-1 in normal mice was rapid, with intact [^11^C]6-OH-BTA-1 composing 73% of the total plasma activity at 2 min after injection and 6% at 30 min. All [^11^C]6-OH-BTA-1 metabolites were polar and are not expected to cross the blood-brain barrier because the brain homogenates at 2 and 10 min contained >95% unmetabolized [^11^C]6-OH-BTA-1.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20primate%20not%20human)]

PET studies were performed in six adult baboons after injection of 185 MBq (5 mCi) of [^11^C]6-OH-BTA-1 or [^11^]BTA-1 and co-registered with MRI anatomical brain images (15). A dynamic series of PET scans were acquired over 60 min. At early time points (0-9 min), radioactivity was uniformly distributed throughout the baboon brains, whereas at the later time points, radioactivity became more heterogeneously distributed. Regions of brain containing higher levels of white matter (such as pons) exhibited 20-30% higher accumulation of radioactivity than regions that were mainly gray matter (such as the temporal, mesial-temporal, and occipital cortex). In the baboon brains, radioactivity concentrations of [^11^C]BTA-1 and [^11^C]6-OH-BTA-1 at 30 min were 0.45 and 0.27% ID-kg/g, respectively. These values were similar to those in mice. [^11^C]6-OH-BTA-1 showed a faster rate of clearance of radioactivity than [^11^C]BTA-1.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-OH-BTA-1%20and%20humans)]

The first human study with [^11^C]6-OH-BTA-1 in 16 patients with mild AD and 9 healthy people was reported (16). The subjects were given an intravenous injection of 300 MBq (8.1 mCi) of [^11^C]6-OH-BTA-1. Plasma metabolism of [^11^C]6-OH-BTA-1 was rapid and similar in the AD patients and normal subjects. The amount of intact [^11^C]6-OH-BTA-1 was 7.2 ± 3.6% (normal control subjects) and 9.8 ± 3.0% (AD) at 60 min after injection. The dynamic PET data showed that [^11^C]6-OH-BTA-1 retention is 1.52-1.94-fold greater in brain regions (such as frontal, parietal, temporal, and occipital cortex and the striatum) that are known to contain amyloid plaques in AD patients than in controls. The frontal cortex had the highest tracer uptake. There was a similar retention of [^11^C]6-OH-BTA-1 in the cerebellum and white matter containing little amyloid deposits in AD and controls. There is an inverse correlation of [^11^C]6-OH-BTA-1 retention with cerebral FDG metabolism in the cortical regions. However, the differences between AD and controls were greater with [^11^C]6-OH-BTA-1 than with FDG.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Mathis C.A., Wang Y., Holt D.P., Huang G.F., Debnath M.L., Klunk W.E. (2003). Synthesis and evaluation of 11C-labeled 6-substituted 2-arylbenzothiazoles as amyloid imaging agents. J Med Chem.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.